# 1-(3,4-[^11^C]Dimethoxyphenethyl)-4-[3-(3,4-dichlorophenyl)propyl]piperazinephenoxy)

Chemical name: | 1-(3,4-[^11^C]Dimethoxyphenethyl)-4-[3-(3,4-dichlorophenyl)propyl]piperazine
Abbreviated name: | [^11^C]SA6298
Synonym:
Agent Category: | Compound
Target: | Sigma (σ) receptor
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal/contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B11C%5DSA6298%20OR%20SA6298)]

1-(3,4-[^11^C]Dimethoxyphenethyl)-4-[3-(3,4-dichlorophenyl)propyl]piperazine ([^11^C]SA6298) is a radioligand developed for positron emission tomography (PET) imaging of the sigma (σ) receptors. [^11^C]SA6298 is a potent σ_1_ receptor agonist labeled with ^11^C, a positron emitter with a physical half-life (t_½_) of 20.4 min (1).

The σ receptors are functional, membrane-bound proteins that are distributed in the central nervous system (CNS) and peripheral organs (2). The CNS σ receptors are unique binding sites related to higher brain functions (3). They are distinct from opiate and phencyclidine binding sites. There are at least two subtypes of σ receptors: σ_1_ and σ_2_ receptors. A σ_3_ receptor subtype has also been proposed (4). The precise mechanism of the functional response of these receptors is not entirely known. These receptors appear to be involved in numerous pharmacological and physiological functions, and they also modulate a number of central neurotransmitter systems, including noradrenergic, glutamatergic, and dopaminergic systems. Phencyclidine and derivatives, cocaine and derivatives, some neuroleptics, atypical antipsychotic agents, and other chemically unrelated compounds can bind to the σ receptor sites. Studies have shown that these receptors may play a role in the pathogenesis of psychiatric disorders (5, 6). These receptors are also expressed on a number of human and murine tumors (7).

The σ_1_ receptor subtypes have a molecular weight of ≈25 kDa, and through the process of cloning they have shown a 30% sequence homology with the yeast C89-C7 sterol isomerase (2, 8, 9) The σ_2_ receptor subtypes have a molecular weight of ≈21.5 kDa and they have not been cloned. The σ_1_ receptors are thought to be involved in certain neuropsychiatric disorders, and the σ_2_ receptors are implicated in malignant neoplastic diseases. Because of these effects, σ receptor ligands may be useful for detection and treatment in neurology and oncology. Matsuno et al. (10) developed a potent σ_1_ agonist, 1-(3,4-dimethoxyphenethyl)-4-(3-phenylpropyl)-piperazine dihydrochloride (SA4503), which is undergoing phase II clinical trials as a therapeutic agent for functional recovery after stroke. SA4503 is highly selective for σ_1_ receptors versus σ_2_ receptors (10). SA5403 can be labeled with ^11^C for PET studies of σ receptors, and studies have shown specific localization of [^11^C]SA4503 in animals and humans (1, 11, 12). SA6298 is an analog of SA4503 with a higher but less selective affinity [inhibition constant (IC_50_) for σ_1_ = 6.9 nM; σ_1_/σ_2_ = 22] for σ_1_ receptors than SA4503 (IC_50_ for σ_1_ = 17.4 nM; σ_1_/σ_2_ = 103) (10, 13, 14). Kawamura et al. (13) evaluated the potential of [^11^C]SA6298 as a PET σ_1_ receptor ligand.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B11C%5DSA6298%20OR%20SA6298%29%20AND%20synthesis)]

Fujimura et al. (14) reported the preparation of SA6298 from phenylpropylamine. Kawamura et al. (13) designed the radiosynthesis of [^11^C]SA6298 based on the precursor desmethyl SA6298 (SA11726), which was obtained commercially. [^11^C]SA6298 was prepared by methylation of SA11726 with [^11^C]CH_3_I. Briefly, [^11^C]CH_3_I was produced with an automated system and trapped in 0.2 ml of N,N-dimethylformamide containing 0.2 mg of SA11726 and 1−4 mg of sodium hydride (NaH). The mixture of SA11726 and NaH was preheated at 80ºC for 2−5 min before [^11^C]CH_3_I was added. The mixture of [^11^C]CH_3_I, SA11726 and NaH was heated at 120ºC for 1 min. The solution was then diluted with a solvent, and [^11^C]SA6298 was isolated by a reversed-phase chromatography. The isolated product was purified by a high-performance liquid chromatography (HPLC). The decay-corrected radiochemical yield (based on [^11^C]CH_3_I) was 38.9 ± 5.2%, and the specific activity (n = 5) was 52.8 ± 16.8 TBq/mmol (453.6 Ci/mmol). The radiochemical purity was >97%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B11C%5DSA6298%20OR%20SA6298%29%20AND%20in%20vitro)]

Fujimura et al. (14) used guinea pig brain homogenate and [^3^H](+)-pentazocine to determine the affinity of SA8298 to σ receptors. The IC_50_ to σ_1_ receptors was 6.9 nM, and the σ_1_/σ_2_ ratio was 22. Kawamura et al. (13) determined that the octanol/phosphate buffered saline partition coefficient of [^11^C]SA6298 was logP_7.4_= 3.82.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B11C%5DSA6298%20OR%20SA6298%29%20AND%20rodentia)]

Biodistribution studies of [^11^C]SA6298 were performed in mice (n = 20) (13). Each mouse received an i.v. dose of 1 MBq(27 μCi) per 25 pmol. The lung showed the highest initial activity level of percent injected dose per g (% ID/g) at 30 min (20.67 ± 1.03%) and then decreased gradually. The radioactivity levels in the brain (1.85 ± 0.08% ID/g at 30 min) and liver (14 ± 0.81% ID/g at 30 min) increased for 60 min. The radioactivity of most other organs (spleen, pancreas, kidney, etc.) increased for the first 15−30 min and then remained constant. Co-injection of unlabeled SA6298 reduced the brain radioactivity to 1.68 ± 0.02% ID/g (30 min) at the dose of 2,000 nmol/kg. The radioactivity levels in the heart, lung, and muscle decreased significantly at doses ≥20 nmol/kg, whereas the blocking effect was found in the spleen, small intestine, liver, and kidney at doses ≥200 nmol/kg. Pretreatment with 2,000 nmol/kg of SA6298 (10 min before) significantly decreased the brain radioactivity level to 1.54 ± 0.08% ID/g. However, postreatment (10 min after) increased the brain level to 4.17 ± 0.36% ID/g. SA4503 and haloperidol at 2,000 nmol/kg also showed a large blocking effect on the brain. Metabolites of [^11^C]SA6298 were analyzed by HPLC and showed that unchanged [^11^C]SA6298 in the brain and plasma was 99 ± 1% and 80 ± 5% (n = 3), respectively, at 30 min after injection.

The receptor-specific uptake of [^11^C]SA6298 was examined in rats (n = 4) (13). Each rat received an i.v. dose of 9.8−10.4 MBq/350 pmol (265−281 μCi/350 pmol). The brain radioactivity levels were reduced to ≈80% of the control by unlabeled SA6298 and SA4503. The levels in the spleen, kidney, and muscle were significantly blocked by both ligands, but the liver level was only blocked by SA6298. Ex vivo autoradiograms of the rat brain after administration of 127−140 MBq/3.6−4.2 nmol (3.4−3.8 mCi/3,6−4.2 nmol) [^11^C]SA6298 (euthanization at 30 min) showed a slightly higher density in the cortex, thalamus, and medial geniculate nucleus. The authors mentioned that cortex and thalamus were known to be rich in σ_1_receptors. The co-injection of unlabeled SA6298 decreased radioactivity in all brain regions by 20−40%.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B11C%5DSA6298%20OR%20SA6298%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

PET imaging was performed in a cat (13) A dose of 197 MBq/4.28 nmol (5.3 mCi/4.28 nmol) was injected intravenously, and the imaging was performed over a period of 60 min. There were high radioactivity levels in the cortex, thalamus, striatum, and cerebellum that remained constant for 60 min. Co-injection of SA6928 (2,000 nmol/kg) decreased these levels by only 10−20% and postinjection of SA6928 did not affect the radioactivity levels. The authors suggested that because of the high affinity of [^11^C]SA6298 for σ_1_ receptors, once it binds to the receptors, it is not easily displaced by the unlabeled SA6298. HPLC analysis of the metabolites showed that unchanged [^11^C]SA6298 in the plasma was 87% at 1 min, 15% at 30 min, and 11% at 60 min. The authors suggested that the lack of a clear specific brain uptake of [^11^C]SA6298 is not explained by the retention of labeled metabolite. The high nonspecific brain binding of [^11^C]SA6298 might be caused by its high lipophilicity

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B11C%5DSA6298%20OR%20SA6298%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B11C%5DSA6298%20OR%20SA6298%29%20AND%20human)]

No publication is currently available.

## References

1 Kawamura K., Ishiwata K., Tajima H., Ishii S., Matsuno K., Homma Y., Senda M. (2000). In vivo evaluation of [(11)C]SA4503 as a PET ligand for mapping CNS sigma(1) receptors. Nucl Med Biol.
2 Lever J.R., Gustafson J.L., Xu R., Allmon R.L., Lever S.Z. (2006). Sigma1 and sigma2 receptor binding affinity and selectivity of SA4503 and fluoroethyl SA4503. Synapse.
3 Skuza G., Wedzony K. (2004). Behavioral pharmacology of sigma-ligands. Pharmacopsychiatry.
4 Myers A.M., Charifson P.S., Owens C.E., Kula N.S., McPhail A.T., Baldessarini R.J., Booth R.G., Wyrick S.D. (1994). Conformational analysis, pharmacophore identification, and comparative molecular field analysis of ligands for the neuromodulatory sigma 3 receptor. J Med Chem.
5 Skuza G. (2003). Potential antidepressant activity of sigma ligands. Pol J Pharmacol.
6 Ishiguro H., Ohtsuki T., Toru M., Itokawa M., Aoki J., Shibuya H., Kurumaji A., Okubo Y., Iwawaki A., Ota K., Shimizu H., Hamaguchi H., Arinami T. (1998). Association between polymorphisms in the type 1 sigma receptor gene and schizophrenia. Neurosci Lett.
7 Vilner B.J., John C.S., Bowen W.D. (1995). Sigma-1 and sigma-2 receptors are expressed in a wide variety of human and rodent tumor cell lines. Cancer Res.
8 Mach R.H., Gage H.D., Buchheimer N., Huang Y., Kuhner R., Wu L., Morton T.E., Ehrenkaufer R.L. (2005). N-[18F]4'-fluorobenzylpiperidin-4yl-(2-fluorophenyl) acetamide ([18F]FBFPA): a potential fluorine-18 labeled PET radiotracer for imaging sigma-1 receptors in the CNS. Synapse.
9 Hanner M., Moebius F.F., Flandorfer A., Knaus H.G., Striessnig J., Kempner E., Glossmann H. (1996). Purification, molecular cloning, and expression of the mammalian sigma1-binding site. Proc Natl Acad Sci U S A.
10 Matsuno K., Nakazawa M., Okamoto K., Kawashima Y., Mita S. (1996). Binding properties of SA4503, a novel and selective sigma 1 receptor agonist. Eur J Pharmacol.
11 Kawamura K., Kubota K., Kobayashi T., Elsinga P.H., Ono M., Maeda M., Ishiwata K. (2005). Evaluation of [11C]SA5845 and [11C]SA4503 for imaging of sigma receptors in tumors by animal PET. Ann Nucl Med.
12 van Waarde A., Buursma A.R., Hospers G.A., Kawamura K., Kobayashi T., Ishii K., Oda K., Ishiwata K., Vaalburg W., Elsinga P.H. (2004). Tumor imaging with 2 sigma-receptor ligands, 18F-FE-SA5845 and 11C-SA4503: a feasibility study. J Nucl Med.
13 Kawamura K., Ishiwata K., Tajima H., Ishii S., Shimada Y., Matsuno K., Homma Y., Senda M. (1999). Synthesis and in vivo evaluation of [11C]SA6298 as a PET sigma1 receptor ligand. Nucl Med Biol.
14 Fujimura K., Matsumoto J., Niwa M., Kobayashi T., Kawashima Y., In Y., Ishida T. (1997). Synthesis, structure and quantitative structure-activity relationships of sigma receptor ligands, 1-[2-(3,4-dimethoxyphenyl)ethyl]-4-(3-phenylpropyl) piperazines. Bioorg Med Chem.